# [^74^As]-Labeled monoclonal antibody against anionic phospholipids

Chemical name: | [^74^As]-Labeled monoclonal antibody against anionic phospholipids
Abbreviated name: | [^74^As]Bavituximab
Synonym: | Monoclonal antibody 3G4
Agent Category: | Monoclonal antibody
Target: | Anionic phospholipids
Target Category: | Antibody-ligand binding
Method of detection: | Positron emission tomography (PET)
Source of Signal/Contrast: | ^74^As
Activation: | No
Studies: | - In vitro; - Rodents | Structure not available.

## Background

[PubMed]

Phospholipids such as phosphatidylserine (PS), phosphatidylinositol, and phosphatidic acid are the most abundant anionic molecules found on the internal surface of the cellular plasma membrane, including that of the vascular tissue (1). Maintenance of the membrane phospholipid topology is an energy-dependent process that involves the ATP-dependent activity of enzymes such as the aminophospholipid translocases, floppases, and scramblases (2, 3). The activity of these enzymes is altered under a variety of pathological conditions and results in the redistribution of membrane phospholipids because PS is exposed to the outer surface of the cell membrane (4). A variety of stress conditions (such as acidity, hypoxia, etc.) and molecules (cytokines, thrombin, oxygen free radicals, etc.), including Ca^2+^ fluxes, have been shown to induce PS exposure on the outer surface of the vascular endothelial cells under in vitro conditions, suggesting that the microenvironment in tumors may be responsible for the altered phospholipid distribution in these lesions (5, 6). Using a monoclonal antibody (mAb) directed toward anionic phospholipids, Ran et al. showed that these charged lipids were also exposed in the solid tumor blood vessel endothelium of mice and suggested that PS could be a specific marker for tumor vasculature (5, 7). Ran et al. subsequently developed another mAb, designated 3G4 or bavituximab, against anionic phospholipids that binds to the target in the presence of serum or the β2-glycoprotein I (8). Bavituximab was shown to destroy tumor blood vessels and slow the growth of tumors in mice.

Advancements in nuclear medicine have made it possible to label antibodies with radionuclides for use as tracers to detect clinically relevant targets, particularly for the treatment of cancers. The major limitation of using labeled antibodies for the detection of targets is that these macromolecules have a prolonged half-life (t_1/2_; i.e. they stay in blood circulation for a long time) and may take a long time to reach optimal concentrations at the target for imaging. Positron emission tomography (PET) is among the several techniques used in nuclear medicine for imaging with nuclides such as copper (^64^Cu), yttrium (^86^Y), or iodine (^124^I), but these radionuclides either have a very short half-life (^64^Cu: t_1/2_ = 12.7 h; ^86^Y; t_1/2_ = 17.8 h) or undergo metabolic dehalogenation (^124^I: t_1/2_ = 4.18 d) from the antibodies; therefore, it is not always suitable to use these nuclides for PET imaging. Although an isotope of arsenic (^74^As: t_1/2_ = 17.8 d) was used for PET imaging of the brain approximately four decades ago (9), the difficulty of isotope production and isolation of the nuclide, along with the lack of a process for the derivatization of the isotope, were major limitations for the popularization of this radioisotope as a PET agent. Advancement in the isolation and use of arsenic isotopes for the labeling of biomolecules has renewed the interest of investigators with regard to the use of this agent for PET imaging (10).

Jennewein et al. labeled bavituximab with ^74^As and evaluated its use for the imaging of solid tumors in rats (10). The United States Food and Drug Administration has approved bavituximab for use in clinical trials to treat advanced tumor malignancies and hepatitis C.

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=Bavituximab+synthesis)]

Ran et al. described the production of bavituximab (8). Briefly, BALB/c mice were immunized with bEnd.3 endothelial cells treated with hydrogen peroxide (H_2_O_2_) (2 h at 37°C). The H_2_O_2_ treatment causes a translocation of the anionic phospholipids to the outer surface of the cell membrane. The mice were injected intraperitoneally with cells five times at three weekly intervals, and hybridomas were obtained by fusing splenocytes from the immunized mice with myeloma partner P3 X 63AG.653 cells. The hybridoma growth medium supernatants were screened for reactivity with PS and other anionic phospholipids immobilized on plastic plates. Bavituximab binds PS through exogenously supplemented β2-glycoprotein I, which acts as a co-factor for the binding. The investigators did not provide any information regarding purification of the mAb before labeling or its use for imaging (8, 10).

The antibodies were modified with N-succinimidyl S-acetylthioacetate (SATA), and the sulfhydryl groups on the mAb were deprotected with hydroxylamine before labeling (10). The thiolated mAb in saline was combined with [^74^As]arsenic chloride ([^74^As]Cl_3_) solution at 37°C for 30 min, and the quality of the labeled antibody was checked with high-performance liquid chromatography (HPLC) on a Bio-select Sec 250-5 column. Stability of radioarsenic-labeled mAb was investigated by incubating the labeled mAb in undiluted fetal bovine serum and analyzing the mixture with HPLC at several time points up to 72 h.

An average of 3.5 thiol groups per molecule of the antibody was added during the SATA modification. The specific activity of the labeled mAb was reported to be >100 GBq/μmol (>2.7 Ci/μmol), and the incubation in serum up to 72 h did not lead to any loss of the isotope from the labeled antibody or degradation of the mAb (10). The radiochemical purity and yield of the labeled mAb was not reported by the investigators (10).

For some work, the isotype-matched control mAb [^74^As]retuximab was used, but the procedure used to prepare the labeled retuximab and its specific activity, radiochemical purity, and radiochemical yield were not reported in the publication (10).

## In Vitro Studies: Testing in Cells and Tissues

[PubMed]

No publications are currently available.

## Animal Studies

### Rodents

[PubMed]

The biodistribution of [^74^As]bavituximab was studied in rats bearing Dunning prostate R3327-AT1 tumors in the left thigh (10). Animals (n = 3 for each agent) were injected intravenously through the tail vein either with [^74^As]bavituximab or [^74^As]rituximab (as a control), and the levels of accumulated radioactivity in the various organs were determined 48 and 72 h after administration. The tumor/normal tissue and the tumor/liver ratios at 72 h were 470 and 22, respectively. The tumor’s accumulated bavituximab/rituximab ratios were 28 and 52 at 48 and 72 h, respectively. On imaging at 24 h after administration of the labeled mAb, the tumors were not clearly distinguishable because of the high body background, but by 72 h the tumors were clearly apparent because the labeled mAb had cleared from blood circulation. Small animal PET showed that [^74^As]bavituximab was localized mainly on the tumor periphery at 48 h with a heterogeneous localization in the central region.

Frozen sections from the tumors and normal tissue were stained to detect human immunoglobulins bound to the cells (10), and the sections were also counterstained with anti-rat CD31 antibodies to detect the vascular endothelium. Images obtained from the two stainings were merged, and a coincidence was observed between the bavituximab and the CD31 antibody. The specificity of bavituximab was confirmed because tumors in rats injected with rituximab did not show any staining in the endothelium. Also, vascular endothelium staining was not observed in the animals’ normal tissues, such as the heart, lungs, liver, pancreas, spleen, brain, and testis. From these studies the investigators concluded that [^74^As]bavituximab was a promising agent for the imaging and detection of tumors.

### Other Non-Primate Mammals

[PubMed]

No publications are currently available.

### Non-Human Primates

[PubMed]

No publications are currently available.

## Human Studies

[PubMed]

No publications are currently available.

## Supplemental Information

[Disclaimers]

## NIH Support

Parts of the studies presented in this chapter were funded by NCI grants CA70907, Pre-ICMIC P20 CA086334, and SAIRP U24 CA126608.

## References

1 van Meer G., Voelker D.R., Feigenson G.W. (2008). Membrane lipids: where they are and how they behave. Nat Rev Mol Cell Biol.
2 Zwaal R.F., Schroit A.J. (1997). Pathophysiologic implications of membrane phospholipid asymmetry in blood cells. Blood.
3 Zhao J., Zhou Q., Wiedmer T., Sims P.J. (1998). Level of expression of phospholipid scramblase regulates induced movement of phosphatidylserine to the cell surface. J Biol Chem.
4 Yamaji-Hasegawa A., Tsujimoto M. (2006). Asymmetric distribution of phospholipids in biomembranes. Biol Pharm Bull.
5 Ran S., Thorpe P.E. (2002). Phosphatidylserine is a marker of tumor vasculature and a potential target for cancer imaging and therapy. Int J Radiat Oncol Biol Phys.
6 Balasubramanian K., Schroit A.J. (2003). Aminophospholipid asymmetry: A matter of life and death. Annu Rev Physiol.
7 Ran S., Downes A., Thorpe P.E. (2002). Increased exposure of anionic phospholipids on the surface of tumor blood vessels. Cancer Res.
8 Ran S., He J., Huang X., Soares M., Scothorn D., Thorpe P.E. (2005). Antitumor effects of a monoclonal antibody that binds anionic phospholipids on the surface of tumor blood vessels in mice. Clin Cancer Res.
9 Bumham C.A., Aronow S., Brownell G.L. (1970). A hybrid positron scanner. Phys Med Biol.
10 Jennewein M., Lewis M.A., Zhao D., Tsyganov E., Slavine N., He J., Watkins L., Kodibagkar V.D., O'Kelly S., Kulkarni P., Antich P.P., Hermanne A., Rosch F., Mason R.P., Thorpe P.E. (2008). Vascular imaging of solid tumors in rats with a radioactive arsenic-labeled antibody that binds exposed phosphatidylserine. Clin Cancer Res.